# (1-(2-(β-Galactopyranosyloxy)propyl)-4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecane) gadolinium(III)

Chemical name: | (1-(2-(β-Galactopyranosyloxy)propyl)-4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecane) gadolinium(III)
Abbreviated name: | EGadMe
Synonym:
Agent category: | Small molecule
Target: | β-Galactosidase
Target category: | Enzyme
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | Yes
Studies: | - In vitro | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EgadMe)]

β-Galactosidase (β-Gal) derived from Escherichia coli (E. coli) is the gene product of the bacterial lacZ operon (1). This 465-kDa tetrameric enzyme is responsible for hydrolysis of lactose and other β-galactosides to monosaccharides (2). β-Gal exhibits fairly strict specificity for sugars in galactosyl positions in a wide variety of aglycones (3). Several chromogenic sugar substrates have been synthetically modified so that their hydrolyzed products are easily detectable by a conventional colorimeter (2, 4). For example, β-Gal hydrolyzes 5-bromo-4-chloro-3-indolyl-β-D-galactoside (X-Gal) to produce a 5-bromo-4-chloro-indigo in blue color (5). The development of substrates like X-Gal makes β-Gal a common enzymatic reporter protein to assay clonal insertions, transcriptional activations, protein expressions, and protein interactions in vitro and in vivo (2, 6). The increase in β-Gal activity in particular has been used as an indirect measure of the enhanced transcription of the lacZ reporter gene (6). A major advantage of using β-Gal as a reporter protein is its high sensitivity originating from efficiently enzymatic turnover (4).

1-(2-(β-Galactopyranosyloxy)propyl)-4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecane) gadolinium(III) (EGadMe) is a modified sugar substrate containing a gadolinium (Gd) chelate (7), which is used to enhance the imaging contrast of β-Gal in magnetic resonance imaging (MRI). EGadMe consists of a high-affinity chelator that occupies eight of the nine coordination sites on Gd^3+^ and a galactopyranose residue that is positioned to block the remaining site on Gd^3+^ from water access. An α-methyl group is attached to the ethylenic carbon on the sugar linkage arm of the tetraazacarboxylic macrocycle to restrict the rotation of the galactopyranose blocking group. As a result, it not only enhances the rigidity of the chelator but also limits the bulk water access to Gd^3+^. The T_1_ relaxivity of Gd chelates contains the contributions from water molecules in two environments: the water molecules that are directly bonded to the metal ions (the inner sphere water) and the water molecules that are not directly bonded to the metal ions (the outer sphere water) (8, 9). For Gd with one structural water (q = 1) in the fast reorientation motion region (small free Gd chelates), the inner sphere water contributes 50–70% to the T_1_ relaxivity depending on the magnetic field strength (8). In the absence of β-Gal, EGadMe is in a water-inaccessible conformation (uncleaved); its T_1_ relaxivity is low because the primary contribution is only from the outer sphere water. The presence of β-Gal enzymatically cleaves the galactopyranose from EGadMe (cleaved), freeing one coordination site (q ~ 1) and causing a substantial increase in the T_1_ relaxivity. Such a substantial change in T_1_ relaxivity allows for measuring the activity of β-Gal by MRI.

Xenopus embryos comprise an important cell system used for biological studies of cell signaling, cell lineage, and cell movement (10). The embryos are typically 1 mm in diameter, which is sufficiently large for easy visualization and manipulation at low magnification. Cell division as early as the stage of the first six divisions generates easily identifiable rows and tiers of cells (blastomeres) (11). A fate map of these blastomeres has been established for identification of the descendents during embryo development (11). The β-Gal gene can be introduced into a Xenopus embryo via transfection of messenger ribonucleic acid (mRNA) of β-Gal or plasmid deoxyribonucleic acid (DNA) carrying the lacZ gene at the two-cell stage (7). At the same time, EGadMe as a MRI lineage tracer is microinjected into both cells, and it remains within the originally labeled cell and its progeny (the descendents) during the growth of embryo. As a result, the transfected cell is easily distinguished from the nontransfected one by MRI and their descendents as well.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( EgadMe)+AND+synthesis%0D%0A)]

Louie et al. reported the details of synthesis of EGadMe in several steps (7). 1-Bromopropan-2-ol was reacted with aceto-1-bromogalactose in the presence of silver trifluoromethanesulfonate (AgOTf) in CH_2_Cl_2_ to yield α- and β-anomers of 2,3,4,6-aceto-1-ethylbromo-galactose. The β-anomer was isolated by flash chromatography and reacted with cyclen to form monosubstituted cyclen. The substituted cyclen was treated with four equivalents of bromoacetic acid to produce the ligand, followed by complexation with GdCl_3_ to yield EGadMe.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( EgadMe)+AND+%22in+vitro%22)]

The water relaxation properties of EGadMe were examined on an 11.7-T magnetic resonance spectrometer (7). The T_1_ relaxivity was found to be 2.72 mM^-1^•s^-1^ for its cleaved conformation and 0.903 mM^-1^•s^-1^ for its uncleaved conformation. The kinetic properties of EGadMe as a substrate of β-Gal were examined in solutions (7). The Michaelis constant (K_m_) of 0.0182 mM and maximum initial velocity (V_m_) of 2.4 × 10^-3^ nmol U^-1^•s^-1^ were extracted from Lineweaver-Burke plots.

The in vivo study of magnetic resonance contrast enhancement was conducted in living X. laevis embryos on an 11.7-T imager (7). Both cells in embryos at the two-cell stage were microinjected with 4 nl of 400 M EGadMe. Then, one of the two cells was transfected with either 4 nl of 0.5-μg/μl mRNA of β-Gal or 4–16 nl of 20-ng/μl linearized plasmid DNA carrying the lacZ gene; the other cell was microinjected with water as a control. Consequently, the transfection led to the generation of ~13,000 copies of the 3,000 bp sequence per cell or ~88–352 copies of the 8.9 kb plasmid per cell in the animal at the 100,000-cell stage. To confirm the MRI labeling, 0.025 μg/μl mRNA of nuclear-localized green fluorescent protein (GFP) was also microinjected into the transfected cells to generate GFP reporter. Both cells contained EGadME, but one existed as the enzymatically processed contrast agent and the other as the unprocessed one. After multiple cell division stages, the two cells developed into the left and right sides of animals. The descendents of the labeled cells remained only on one side as predicted by the embryo development fate map for (11). As a result, the images of the embryo injected with both β-Gal mRNA and EGadMe (cleaved) demonstrated an expected increase in signal intensity compared to that of the embryo injected with EGadMe alone (uncleaved). A significant signal intensity enhancement of MRI (57%) was found on the side that expressed β-Gal compared to the equivalent somites on the other side that did not express β-Gal. This result was further confirmed by light microscopy of the embryo fixation with X-Gal staining and nuclear-localized GFP fluorescence measurement. In the embryo transfected with plasmid DNA of the lacZ gene, the magnetic resonance image correlated well with the image of the same embryo after fixation and staining with X-Gal.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( EgadMe) +AND++rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( EgadMe) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( EgadMe) +AND+human)]

No publication is currently available.

### NIH Support

AR 42671, AI 47003, DA 08944, RR 13625, GM 20526

## References

1 Juers D.H., Jacobson R.H., Wigley D., Zhang X.J., Huber R.E., Tronrud D.E., Matthews B.W. (2000). High resolution refinement of beta-galactosidase in a new crystal form reveals multiple metal-binding sites and provides a structural basis for alpha-complementation. Protein Sci.
2 Serebriiskii I.G., Golemis E.A. (2000). Uses of lacZ to study gene function: evaluation of beta-galactosidase assays employed in the yeast two-hybrid system. Anal Biochem.
3 Matthews B.W. (2005). The structure of E. coli beta-galactosidase. C R Biol.
4 Eglen R.M., Singh R. (2003). Beta galactosidase enzyme fragment complementation as a novel technology for high throughput screening. Comb Chem High Throughput Screen.
5 Mohler W.A., Blau H.M. (1996). Gene expression and cell fusion analyzed by lacZ complementation in mammalian cells. Proc Natl Acad Sci U S A.
6 Rossi F., Charlton C.A., Blau H.M. (1997). Monitoring protein-protein interactions in intact eukaryotic cells by beta-galactosidase complementation. Proc Natl Acad Sci U S A.
7 Louie A.Y., Huber M.M., Ahrens E.T., Rothbacher U., Moats R., Jacobs R.E., Fraser S.E., Meade T.J. (2000). In vivo visualization of gene expression using magnetic resonance imaging. Nat Biotechnol.
8 Lauffer R.B. (1987). Paramagnetic metal complexes as water proton relaxation agents for NMR imaging:Theory and design. Chem. Rev.
9 Caravan P., Ellison J.J., McMurry T.J., Lauffer R.B. (1999). Gadolinium(III) Chelates as MRI Contrast Agents: Structure, Dynamics, and Applications. Chem Rev.
10 DeSimone D.W., Dzamba B., Davidson L.A. (2007). Using Xenopus embryos to investigate integrin function. Methods Enzymol.
11 Walmsley M., Ciau-Uitz A., Patient R. (2005). Tracking and programming early hematopoietic cells in Xenopus embryos. Methods Mol Med.